# (S)-N,N’-bis[2-hydroxy-1-(hydroxymethyl)-ethyl-2,4,6-triiodo-5-lactamidoisophthalamide

Chemical name: | (S)-N,N’-bis[2-hydroxy-1-(hydroxymethyl)-ethyl-2,4,6-triiodo-5-lactamidoisophthalamide
Abbreviated name:
Synonym: | Iopamidol, Isovue
Agent Category: | Compound
Target: | Blood pool, extracellular fluid space
Target Category: | Nonspecific filling of extracellular fluid space
Method of detection: | CT and X-ray
Source of signal: | Iodine
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Iopamidol)]

Computed tomography (CT) is a diagnostic imaging procedure that uses a combination of x-rays and computer technology to produce cross-sectional images used to diagnose or evaluate treatment of a variety of the cardiovascular system diseases, peripheral angiography, and cancer. This is a noninvasive technique and may require the administration of a contrast media (CM) before the procedure is performed. The CMs used for these procedures are usually iodinated compounds and are classified as ionic or nonionic on the basis of their chemistry. Both CM varieties are either high- or low-osmolality and are available in monomeric or dimeric forms (1). The CM preparations are usually available at various iodine concentrations and have different physiochemical properties such as pH, hydrophilicity, and viscosity. Although CMs are considered safe to use, some patients may experience a general adverse reaction or nephrotoxicity with these agents (1-4). The management of these reactions has been discussed, and different methods to reduce development of toxicity in the patients have been proposed by some investigators (3-5). The nonionic variety of CMs was developed because the ionic variety had a higher rate of adverse reactions and was particularly unsuitable for severely ill patients or individuals with kidney dysfunction (2, 4).

This chapter is a brief review of (S)-N,N’-bis[2-hydroxy-1-(hydroxymethyl)-ethyl-2,4,6-triiodo-5-lactamidoisophthalamide (generic name: iopamidol), an iodinated, nonionic, low-osmolality CM. Iopamidol was approved for use as a CM by the US Food and Drug Administration and is commercially available in the US. According to the manufacturer (6), this CM may be used for adult and pediatric angiography throughout the cardiovascular system, coronary arteriography and ventriculography, intravenous excretory urography, contrast enhancement of CT (CECT), and head and body imaging.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=iopamidol%20synthesis)]

The method to synthesize iopamidol has been described in a patent issued to the manufacturer in the US (7).

For this, N,N’-bis[2-(acetyloxy)-1-[(acetyloxy)methyl]ethyl]-5-amino-2,4,6-triiodo-1-,3-benzenedicarboxamide was mixed with dimethylacetamide (DMA). A solution of propanediol and triethylamine in DMA was then added to the mixture. After mixing, the temperature was gradually elevated to 30°C and maintained for 1.5 h. The reaction was then cooled, and 4-dimethylaminopyridine was added to the vessel and followed by slow addition of acetic anhydride. The mixture was stirred for 2 h and quenched by slow addition of water to yield a solid. The solid was isolated by filtration, washed with water, and dried, with a yield of 90%. The solid was dissolved in DMA and 2(S)-acetoxypropionyl chloride was slowly added to it. The reaction was stirred at room temperature for ~2 h and quenched by the slow addition of isopropanol to obtain pentaacetyliopamidol. The pentaacetyliopamidol was collected by filtration, washed with isopropanol, and dried, with a yield of 90%. A solution of pentaacetyliopamidol in methanol was refluxed for ~30 h with aqueous hydrochloric acid. The methanol was removed by distillation and the residue was dissolved in water. The residual acid was neutralized by stirring the solution with an acid-scavenging resin. The resin was removed by filtration and the aqueous solution was passed through a column of Amberlite XDA-16 resin. The eluent was concentrated to obtain an oil and a residue that was crystallized by heating the oil in a mixture of acetonitrile and ethanol. Iopamidol was collected by filtration, washed with ethanol, and dried. The yield was 74%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=iopamidol%20in%20vitro)]

Because of the intra-arterial or intravenous application of iopamidol, a variety of studies describing the in vitro effects of this agent on cell adhesion molecules (8), platelet aggregation (9), partial thromboplastin time (10), thrombogenicity (11), potassium release rates in blood (12), metabolic functions in renal epithelial cells (13, 14), nephrotoxicity (15), and chemotoxic effects on renal tubules (16) are available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Iopamidol%20rodentia)]

The use of iopamidol was compared with a new contrast agent, Fenestra VC, for in vivo imaging of cardiac structure and function in mice (17). Fenestra VC is a contrast agent that consists of iodinated triglycerides formulated in a stable, oil-in-water lipid emulsion. One group of mice received a constant infusion of iopamidol while the other group received a single bolus injection of Fenestra VC. The investigators observed and concluded that Fenestra VC was a better contrast agent compared to iopamidol to study cardiac structure and function in these animals because it provided a higher signal-to-noise ratio.

The use of CM diffusion across vascular endothelium to study the magnitude of endothelial defects induced by the endotoxin lipopolysaccharide (LPS) sepsis was evaluated in a rat model (18). LPS was administered to the animals through the intraperitoneal route, and the vascular leakage and volume values were quantified in the various organs (myocardium, kidney, liver, and colonic wall) after the administration of various CMs, including iopamidol. Vascular leakage increased in all the organs and the elimination of iopamidol from the intravascular compartment in LPS-treated animals was reduced compared with controls. The investigators concluded that CMs could be used to study vascular leakage and volume in an animal model of endotoxin toxicity.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Iopamidol%20Non-Primate%20Mammals)]

The use of rabbits to determine nephrotoxicity of several ionic and nonionic CMs, including iopamidol, has been described (19). Nonionic monomer CMs were observed to be nephrotoxic at ~15 times the normal dose used for CT procedures.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Iopamidol%20Non-Human%20Primates)]

The distribution of therapeutics to specific locations in the central nervous system is often performed by using the convection-enhanced delivery (CED) system (20). The system requires use of surrogate imaging tracers to monitor optimal, real-time, in vivo distribution of drugs. Using CED, Croteau et al. (20) used clinical observations and histopathology of the animals to evaluate the safety and toxicity of iopamidol as a surrogate tracer for CT scanning of the central nervous system in primates (Macaca mulatta). Distribution of the tracer in the animals was determined by in vivo real-time and postinfusion CT scanning along with quantitative autoradiography using ^14^C sucrose and ^14^C dextran. The investigators concluded that iopamidol was safe and suitable for monitoring drug delivery using CED and produced no clinical or histopathological toxicity in the animals.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=iopamidol%20human%20studies)]

The use of iopamidol for different techniques has been investigated in various clinical studies [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=iopamidol%20clinical%20trials)] designed to diagnose cancer [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=iopamidol%20cancer)], investigate cardiac function [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=iopamidol%20cardiac%20function)], vasculature [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=iopamidol%20vasculature)], and nephrotoxicity [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=iopamidol%20nephrotoxicity)].

Iopamidol was used as an alternative to radioactivity for interstitial CT lymphography in superficial esophageal cancer patients (21). Sentinel lymph node (SLN) mapping and biopsy examination was performed on the patients using an experimental endoscopic CT technique after an endoscopic submucosal peritumoral injection of iopamidol. This was followed by radical esophagectomy and regional lymph node dissection with CT lymphography guidance. The draining lymphatic vessels and the SLNs were visualized by CT within 5 min of CM injection and the lymph node metastasis was detected with excellent accuracy and sensitivity. The investigators concluded although this study (21) showed that endoscopic CT lymphography using iopamidol could be clinically applied for esophageal SLN mapping and biopsy examination, a larger investigation would be necessary to establish its accuracy and usefulness.

Murakami et al. (22) investigated the use of iopamidol with a double-phase CT technique for the diagnosis of hepatocellular carcinoma. With results obtained from the study, the investigators concluded that the technique could improve diagnostic accuracy of cancer detection.

Bone marrow transplantation (BMT) patients are often exposed to a variety of nephrotoxic, antineoplastic, immunosuppressive, and antimicrobial drugs. In addition, BMT patients are also often subjected to CT using low-osmolality CMs to detect any infections or other non-hematological complications. The clinical records of 120 pediatric patients who had undergone allogenic BMT were reviewed to assess the effects of iopamidol and antimicrobial drugs on the renal function of these individuals (23). Serum creatinine and blood urea nitrogen concentrations were measured 24 h before and 72 h after each administration of iopamidol for CT examination performed within 100 days of BMT. The reviewers concluded that iopamidol had negligible nephrotoxicity in the allogenic pediatric BMT patients, even in individuals with elevated renal function prior to the procedure.

An estimated 0.6–2.3% of patients who undergo an angiographic procedure may experience contrast-induced nephropathy (CIN), and the incidence is particularly higher (3.3–14.5%) in patients with cardiovascular problems (24). Patients with impaired renal function, diabetes, or a combination of the two are also a population at high risk for CIN (25). It is believed that CIN is the result of direct CM toxicity to the renal tubular cells and medullary ischemia. Although CM osmolality is generally considered as the main cause of nephrotoxicity, other factors, such as molecular structure differences of the CM (26) and free radical generation (27), also probably contribute to the development of CIN. A review of data obtained from several clinical trials where CMs were used for cardiac or peripheral angiography showed that iopamidol had a lower incidence of CIN compared to other CMs (24, 28). The antioxidant acetylcysteine was shown to reduce renal ischemic failure in animals (29), and Kay et al (30). investigated the prophylactic use of this compound to prevent CIN in patients with moderate renal insufficiency undergoing coronary angiography with iopamidol. From this study the investigators concluded that acetylcysteine was a safe, effective, and inexpensive prophylactic treatment against CIN. In contrast, another study (31) concluded that there was no benefit of the prophylactic treatment with acetylcysteine for patients undergoing peripheral angiography with CMs, including iopamidol. In another study to evaluate the prophylactic treatment of sodium bicarbonate or sodium chloride against CIN caused by iopamidol, it was concluded that sodium bicarbonate was more effective than sodium chloride in reducing the occurrence of CIN (32).

## References

1 Morcos S.K., Thomsen H.S. (2001). Adverse reactions to iodinated contrast media. Eur Radiol.
2 Katayama H., Yamaguchi K., Kozuka T., Takashima T., Seez P., Matsuura K. (1990). Adverse reactions to ionic and nonionic contrast media. A report from the Japanese Committee on the Safety of Contrast Media. Radiology.
3 Morcos S.K., Thomsen H.S., Webb J.A. (2001). Prevention of generalized reactions to contrast media: a consensus report and guidelines. Eur Radiol.
4. Stacul, F., Managing the risk associated with use of contrast media for computed tomography. Eur J Radiol, 2007.
5 Thomsen H.S., Morcos S.K. (2004). Management of acute adverse reactions to contrast media. Eur Radiol.
6. Inc., B.D., Isovue Multipack. 2004, Bracco diagnostics, Inc.: Princeton, NJ.
7. Lorenzini, R.A., A.V. Bhatia, S.A. Chamberlin, K.A. Drengler, J.J. Hufnagel, and X.C. Wang, Process for the preparation of iopamidol., in Unnited States Patent number 7,115,778, U.S.P. Office, Editor. 2006, Bracco Imaging, S. p. A.: United States of America.
8 Zhan X., Agrawal D.K., Thorpe P.E. (1998). Effect of iodinated contrast media on neutrophil adhesion to cultured endothelial cells. J Vasc Interv Radiol.
9 Heptinstall S., White A., Edwards N., Pascoe J., Sanderson H.M., Fox S.C., Henderson R.A. (1998). Differential effects of three radiographic contrast media on platelet aggregation and degranulation: implications for clinical practice?. Br J Haematol.
10 Gritli N., Nsiri B., Mazigh C., Ghazouani E., M'Henni H., Machghoul S., Gueddiche M. (1998). Anticoagulant profile of iopamidol and meglumine amidotrizoate and their lack of thrombin generation: an in vitro study. Pathol Biol (Paris).
11 Fauser C., Ullisch E.V., Kubler W., Haller C. (2001). Differential effects of radiocontrast agents on human umbilical vein endothelial cells: cytotoxicity and modulators of thrombogenicity. Eur J Med Res.
12 Hayakawa K., Nakamura T., Shimizu Y. (2002). Iodinated contrast medium-induced potassium release: the effect of mixing ratios. Radiat Med.
13 Nakamura M., Uozumi J., Soejima K., Kanou T., Tokuda N., Naito S. (2003). Inhibition of gluconeogenesis and p-aminohipuric acid accumulation in rat renal cortical slices by ionic and nonionic contrast media. Clin Exp Nephrol.
14 Soejima K., Uozumi J., Kanou T., Fujiyama C., Masaki Z. (2003). Nonionic contrast media are less nephrotoxic than ionic contrast media to rat renal cortical slices. Toxicol Lett.
15 Rauch D., Drescher P., Pereira F.J., Knes J.M., Will J.A., Madsen P.O. (1997). Comparison of iodinated contrast media-induced renal vasoconstriction in human, rabbit, dog, and pig arteries. Invest Radiol.
16 Hardiek K., Katholi R.E., Ramkumar V., Deitrick C. (2001). Proximal tubule cell response to radiographic contrast media. Am J Physiol Renal Physiol.
17 Badea C.T., Fubara B., Hedlund L.W., Johnson G.A. (2005). 4-D micro-CT of the mouse heart. Mol Imaging.
18 Langheinrich A.C., Ritman E.L. (2006). Quantitative imaging of microvascular permeability in a rat model of lipopolysaccharide-induced sepsis: evaluation using cryostatic micro-computed tomography. Invest Radiol.
19 Pettersson G. Towart R. Grant D. Thyberg K. Golman K. The rabbit renal toxicity test: a sensitive in vivo test for the nephrotoxicity of contrast agents Acad Radiol 2002 9 Suppl 1 S62 4 12019897
20 Croteau D., Walbridge S., Morrison P.F., Butman J.A., Vortmeyer A.O., Johnson D., Oldfield E.H., Lonser R.R. (2005). Real-time in vivo imaging of the convective distribution of a low-molecular-weight tracer. J Neurosurg.
21 Hayashi H., Tangoku A., Suga K., Shimizu K., Ueda K., Yoshino S., Abe T., Sato T., Matsunaga N., Oka M. (2006). CT lymphography-navigated sentinel lymph node biopsy in patients with superficial esophageal cancer. Surgery.
22 Murakami T., Takamura M., Kim T., Hori M., Federle M.P., Onishi H., Tomoda K., Nakamura H. (2005). Double phase CT during hepatic arteriography for diagnosis of hepatocellular carcinoma. Eur J Radiol.
23 Haight A.E., Kaste S.C., Goloubeva O.G., Xiong X.P., Bowman L.C. (2003). Nephrotoxicity of iopamidol in pediatric, adolescent, and young adult patients who have undergone allogeneic bone marrow transplantation. Radiology.
24 Solomon R. (2005). The role of osmolality in the incidence of contrast-induced nephropathy: a systematic review of angiographic contrast media in high risk patients. Kidney Int.
25 McCullough P.A., Wolyn R., Rocher L.L., Levin R.N., O'Neill W.W. (1997). Acute renal failure after coronary intervention: incidence, risk factors, and relationship to mortality. Am J Med.
26 Heinrich M., Uder M. (2006). Nephrotoxicity of low-osmolar and iso-osmolar contrast media. Kidney Int.
27 Katholi R.E., Woods W.T., Taylor G.J., Deitrick C.L., Womack K.A., Katholi C.R., McCann W.P. (1998). Oxygen free radicals and contrast nephropathy. Am J Kidney Dis.
28 Solomon R., Dumouchel W. (2006). Contrast media and nephropathy: findings from systematic analysis and Food and Drug Administration reports of adverse effects. Invest Radiol.
29 Salom M.G., Ramirez P., Carbonell L.F., Lopez Conesa E., Cartagena J., Quesada T., Parrilla P., Fenoy F.J. (1998). Protective effect of N-acetyl-L-cysteine on the renal failure induced by inferior vena cava occlusion. Transplantation.
30 Kay J., Chow W.H., Chan T.M., Lo S.K., Kwok O.H., Yip A., Fan K., Lee C.H., Lam W.F. (2003). Acetylcysteine for prevention of acute deterioration of renal function following elective coronary angiography and intervention: a randomized controlled trial. Jama.
31 Sandhu C., Belli A.M., Oliveira D.B. (2006). The role of N-acetylcysteine in the prevention of contrast-induced nephrotoxicity. Cardiovasc Intervent Radiol.
32 Merten G.J., Burgess W.P., Gray L.V., Holleman J.H., Roush T.S., Kowalchuk G.J., Bersin R.M., Van Moore A., Simonton C.A., Rittase R.A., Norton H.J., Kennedy T.P. (2004). Prevention of contrast-induced nephropathy with sodium bicarbonate: a randomized controlled trial. Jama.